# 5-[^18^F]Fluoro-2-(1-methyl-1H-pyrrolo[2,3-b]pyridin-5-yl)-oxazolo[5,4-b]pyridine

Chemical name: | 5-[^18^F]Fluoro-2-(1-methyl-1H-pyrrolo[2,3-b]pyridin-5-yl)-oxazolo[5,4-b]pyridine
Abbreviated name: | [^18^F]MK-3328
Synonym:
Agent Category: | Compound
Target: | β-amyloid plaques
Target Category: | Protein
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=beta%20amyloid&cmd=DetailsSearch)]

The gradual development and worsening of dementia is a characteristic feature of Alzheimer’s disease (http://www.alz.org/alzheimers_disease_what_is_alzheimers.asp) (AD), and currently no cure is available for this ailment. Medications available to treat AD can only modify or delay the onset of this disease, and there are many ongoing preclinical and clinical studies to develop a suitable therapy to treat this condition (1). It is hypothesized (known as the amyloid cascade hypothesis) that accumulation of an amyloid precursor protein derivative, the β-amyloid protein (Aβ), in the brain is responsible for bringing about changes in the biochemical and cellular functions of the brain and leads to the progression and manifestation of AD (2). Therefore, the Aβ is believed to be a good biomarker for the detection of AD. Most earlier studies performed to investigate this disease used human post-mortem brains, and little is known about the early events that promote the development of AD or about how the formation and deposition of the Aβ contributes to the disease process (2). More recently, many noninvasive imaging probes that can be used with the various imaging modalities, have been developed and evaluated for the detection of early stage Aβ plaques; however, due to inadequate permeation across the blood–brain barrier and/or low binding to the Aβ aggregates, these agents were considered unsuitable for visualization of the Aβ plaques in the human brain (2).

In an effort to develop imaging compounds that can be used for the visualization of Aβ plaques, investigators have produced and evaluated radiolabeled compounds that can be used with positron emission tomography (PET) (3). Among these, the ^11^C-labeled Pittsburg Compound-B ([^11^C]PIB), which has been shown to bind specifically to Aβ deposits in post-mortem AD brains under in vitro conditions, is most commonly used to diagnose the condition, but the major limitation of using this probe is the short half-life of ^11^C (t_1/2_ = 20 min) and the requirement of an onsite cyclotron for the generation of this radionuclide (2, 3). AS a result, ^11^C-labeled tracers are not the most suitable for commercialization (4), and [^11^C]PIB is not approved by the United States Food and Drug Administration (FDA) as a diagnostic imaging agent for the detection of AD. ^18^F-Labeled AV-45 ([^18^F]AV-45), which has a t_1/2_ = 110 min and has been developed, characterized, and evaluated for the detection of Aβ plaques, has been shown to be suitable for the identification of patients with AD, and the binding of this tracer in the brain of AD patients correlated well with the presence of Aβ plaques observed in this organ during post-mortem studies (5). However, [^18^F]AV-45 is not approved by the FDA as yet for the detection of AD in patients. Although [^18^F]AV-45 (http://www.fda.gov/downloads/AdvisoryCommittees/CommitteesMeetingMaterials/Drugs/PeripheralandCentralNervousSystemDrugsAdvisoryCommittee/UCM240266.pdf) appears to be a promising agent for the noninvasive detection of Aβ plaques, it may not be suitable for the visualization of early-onset Aβ deposits because this tracer (and other similar agents) shows high uptake in the white matter of the brain (3, 5). In a continued effort to develop an imaging agent that is superior to those currently available for the detection of Aβ deposits, Hostetler et al. developed 5-[^18^F]fluoro-2-(1-methyl-1H-pyrrolo[2,3-b]pyridin-5-yl)-oxazolo[5,4-b]pyridine ([^18^F]MK-3328) and showed that it was a promising PET agent for the detection of Aβ plaques because it has a low in vivo uptake in the white matter and the cortical gray matter of the rhesus monkey brain (3).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

β-Amyloid (A4) precursor protein gene information (http://www.ncbi.nlm.nih.gov/gene/351) (Gene ID 351)

Information in Online Mendelian Inheritance in Man (OMIM) Database (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=Amyloid) related to β-amyloid plaques

Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16) on U.S. Food and Drug Administration web site

Partial structure of β-amyloid protein (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=92080) (Protein Data Bank, NCBI)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of MK-3328 has been described by Harrison et al. (6), and its labeling with [^18^F]fluoride is detailed by Hostetler et al. (3). The average yield of [^18^F]MK-3328 was reported to be 14 ± 13%, with a specific activity of 91.5 ± 51.4 GBq/mmol (2,471 ± 1,389 Ci/mmol) and a radiochemical purity (RP) of >98% (n = 25 synthesis reactions).

For comparison purposes, some other ^18^F-labeled compounds were synthesized and studied (3). These radiolabeled compounds are listed in Table 1 below:

Table 1: Comparison of radiolabeled compounds

Radiolabeled compound | Yield | Specific activity (per mmol) | Radiochemical purity | Number of synthesis performed
[^18^F]-AD-278 | 40 ± 18% | 38.2 GBq (1,032 Ci) | >99% | 2
[^18^F]AD-269 | 35 ± 18% | 186 ± 108 GBq (5,023 ± 2,927 Ci) | >99% | 4
[^18^F]AD-265 | 10 ± 3% | Not reported | >98% | 2
[^18^F]AV-45 | 39% | 36.8 GBq (994 Ci) | >98% | 1

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-MK%203328%20in%20vitro&cmd=DetailsSearch)]

The lipophilicity (Log D) of various Aβ ligands was determined as described by Hostetler et al. (3). The Log D values for the various Aβ binding compounds (Table 2 below) were higher (ranging from 2.91 for MK-3328 to 3.52 for AD-265) than that of PIB (Log D = 2.23).

Table 2: Lipophilicity and in vitro binding characteristics of various Aβ binding compounds

Compound | Lipophilicity (Log D) | Binding affinity (IC _ 50 _ in nM)
MK-3328 | 2.91 | 10.5 ± 1.3
AD-269 | 3.42 | 8.0 ± 3.7
AD-278 | 3.52 | 4.0 ± 3.7
AD-265 | 3.03 | 17.0*
PIB | 2.23 | 2.3 ± 0.17

*Single determination.

In a competition binding assay using brain frontal cortex homogenates (controls) of AD patients ([^3^H_3_]DMAB was used as the binding ligand), the Log D values and IC_50_ concentrations of various nonradioactive Aβ binding compounds were compared (Table 2) (6). From this assay it was clear that all the compounds except PIB had a low affinity for the homogenates and that AD-265 was the least potent ligand. The absence of Aβ plaques in the homogenates was confirmed with immunostaining. This suggested that the low-affinity compounds (MK-3328, AD-269, and AD-278) showed no specific binding to the control brain homogenates. In addition, none of the compounds were determined to be unsuitable substrates for the P-glycoprotein transporter, and all of them had suitable cell permeability rates (for details, see Hostetler et al. (3).

Hostetler et al. compared the binding of [^3^H]MK-3328 (5 nM) and [^3^H]AD-269 (5 nM) to Aβ deposits in human AD donor brain slices with autoradiography of the brain slice exposure to the two labeled compounds (3). From the autoradiographic images it was clear that only [^3^H]MK-3328 bound to the amyloid deposits in the frontal cortex of the diseased human brain. In a self-blocking experiment, nonradioactive MK-3328 was shown to completely block the binding of [^3^H]MK-3328 to the Aβ plaques in the AD donor brain slices. In addition, [^3^H]MK-3328 showed no binding in the cerebellum of an AD patient brain (the cerebellum of the AD patient brain is known to have very few Aβ plaque deposits). Similarly, [^3^H]MK-3328 did not show any binding to the frontal cortex of a non-AD human donor brain. From this study the investigators concluded that the specific binding of [^3^H]MK-3328 to the Aβ plaques was probably due to its lower lipophilicity (Log D = 2.91) compared with that of [^3^H]AD-269 (Log D = 3.42).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DMK-3328%20rodentia&cmd=DetailsSearch)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DMK-3328%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DMK-3328%20Non-Human%20Primates&cmd=DetailsSearch)]

The in vivo evaluation of [^18^F]MK-3328 and the other Aβ PET tracers was not performed in transgenic rodents that produce Aβ plaques in their brains because probes that can be used for the imaging of AD in humans do not generate a specific signal in these animals (3). It has been shown that PIB does not have a high affinity for Aβ plaques in the chimpanzee or rhesus monkey brain (3). Therefore, the investigators studied the brain uptake and subsequent kinetics of [^18^F]MK-3328 and the other Aβ plaque-binding PET tracers to establish which one of these agents was the most suited for further studied. Because Aβ plaques are present mostly in the gray matter areas of the human AD brain, the investigators concluded that a comparative analysis of tracer uptake in the white and gray matter of the monkey brain could provide a clue to the selection of a suitable imaging agent for the imaging of Aβ deposits.

Harrison et al. studied the brain uptake and kinetics of [^18^F]MK-3328 in a healthy rhesus monkey (under anesthesia) with PET imaging (6). The route of administration and the amount of tracer injected into the monkey were not reported. From the PET images it was observed that the peak uptake values of the tracer in the cortex and the cerebellum of the brain were ~2.7 and ~3.0 standardized uptake value units, respectively, and in both areas of the brain the tracers were reduced to ~50% of the peak value at 45–90 min. The investigators concluded that, because the Aβ plaques in human AD brain are present throughout the brain but not in the cerebellum until the last stages of the disease, the cerebellum could be used as a suitable baseline reference region for imaging studies.

In another study, two rhesus monkeys (numbers R352 and R460) under anesthesia were used for the brain uptake and washout kinetics studies of the different Aβ deposit binding PET agents (3). The route of administration and the amount of tracer injected into each monkey were not reported. Baseline reference PET scans were obtained with [^18^F]MK-3328, [^18^F]AD-269, and [^18^F]AD-278 in both the monkeys; with [^18^F]AD-265 and [^18^F]AV-45, the scans were acquired from monkey R352 only. Time-activity curves generated from the PET images showed that peak uptake values of the labeled compounds in the cerebellum ranged from 2.4 to 3.2 SUV. In general, the peak uptake was lower in the white matter than in the gray matter (the cortex and cerebellum), but at later time points the white matter showed a higher retention of label compared with the cortical tissues. Similar kinetics of tracer uptake and washout were observed in the cerebellum and the cortex; both tissues showed a rapid washout of radioactivity. Using Logan graphical analysis with the cerebellum cortex as the reference point, the binding potentials (BP) of the various tracers were determined (Table 3) from the PET images as described by Hostetler et al. (3).

Table 3: Binding potential of various Aβ plaque PET imaging agents in cortex and white matter of monkeys

[ ^ 18 ^ F]-Tracer | Monkey R352 | | Monkey R460
[ ^ 18 ^ F]-Tracer | Binding potential
[ ^ 18 ^ F]-Tracer | Cortex | White matter | Cortex | White matter
[ ^ 18 ^ F]MK-3328 | 0.13 | 0.15 | 0.10 | 0.08
[ ^ 18 ^ F]AD-269 | 0.15 | 0.15 | 0.08 | 0.12
[ ^ 18 ^ F]AD-278 | 0.13 | 0.34 | 0.08 | 0.19
[ ^ 18 ^ F]AD-265 | 0.22 | 0.55 | – | –
[ ^ 18 ^ F]AV-45 | 0.11 | 0.33 | – | –

Among the different PET agents, the highest BP in the cortex and the white matter was observed with [^18^F]AD-265. [^18^F]AD-278 and [^18^F]AV-45 showed a similar trend, with a low BP in the cortex but a high BP in the white matter. Compared with the other tracers, both [^18^F]MK-3328 and [^18^F]AD-269 had a lower BP in the cortex and the white matter, indicating that these tracers were probably most suitable for the imaging of Aβ plaques. The observations with [^18^F]MK-3328 and [^18^F]AD-269 were subsequently confirmed in a second monkey (monkey R460). Although [^18^F]MK-3328 and [^18^F]AD-269 had similar BP values, [^18^F]AD-269 had a higher lipophilicity than [^18^F]MK-3328 (see Table 2 above).

With results obtained from the in vitro and in vivo studies described above, the investigators concluded that [^18^F]MK-3328 was superior to all the other Aβ PET agents evaluated in this study, but further evaluation is needed before [^18^F]MK-3328 can be used for the detection of AD in humans (3).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DMK-3328%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Karran E., Mercken M., De Strooper B. (2011). The amyloid cascade hypothesis for Alzheimer's disease: an appraisal for the development of therapeutics. Nat Rev Drug Discov.
2 Quigley H., Colloby S.J., O'Brien J.T. (2011). PET imaging of brain amyloid in dementia: a review. Int J Geriatr Psychiatry.
3 Hostetler E.D., Sanabria-Bohorquez S., Fan H., Zeng Z., Gammage L., Miller P., O'Malley S., Connolly B., Mulhearn J., Harrison S.T., Wolkenberg S.E., Barrow J.C., Williams D.L., Hargreaves R.J., Sur C., Cook J.J. (2011). [(18)F]Fluoroazabenzoxazoles as potential amyloid plaque PET tracers: synthesis and in vivo evaluation in rhesus monkey. Nucl Med Biol.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Wong D.F., Rosenberg P.B., Zhou Y., Kumar A., Raymont V., Ravert H.T., Dannals R.F., Nandi A., Brasic J.R., Ye W., Hilton J., Lyketsos C., Kung H.F., Joshi A.D., Skovronsky D.M., Pontecorvo M.J. (2010). In vivo imaging of amyloid deposition in Alzheimer disease using the radioligand 18F-AV-45 (florbetapir [corrected] F 18). J Nucl Med.
6 Harrison S.T., Mulhearn J., Wolkenberg S.E., Miller P.J., O’Malley S.S., Zeng Z., Williams J. (2011). D. L., E.D. Hostetler, S. Sanabria-Bohórquez, L. Gammage, H. Fan, C. Sur, J.C. Culberson, R.J. Hargreaves, J.J. Cook, J.D. Hartman, and J.C. Barrow, Synthesis and Evaluation of 5-Fluoro-2-aryloxazolo[5,4-b]pyridines as β-Amyloid PET Ligands and Identification of MK-3328. ACS Medicinal Chemistry Letters.